# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 minibody

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 minibody
Abbreviated name: | ^111^In-DOTA-T84.66 minibody
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8). ^99m^Tc-Arcitumomab, a murine anti-CEA mAb Fab’ fragment, was developed for use in single-photon emission computed tomography (SPECT) imaging of CEA expression.

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) and the minibody fragment (a dimer of scFvs-C_H_3 with linker comprising 18 amino acids (GS18); molecular mass = 80 kDa) have been evaluated for targeting in several tumor antigen systems and have demonstrated rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 antibodies, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. A T84.66 minibody was conjugated with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and radiolabeled with ^111^In for localization of CEA-positive tumors in mice (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20synthesis)]

A mixture of recombinant T84.66 minibody and N-hydroxysuccinimidyl-DOTA in a 1:1,000 molar ratio was incubated at 4°C for 18 h (14, 15). The DOTA/diabody ratio was determined to be >1. The DOTA-minibody (~5 nmol) was incubated with 48.1 MBq (1.3 mCi) ^111^InCl_3_ in 0.25 NH_4_OAc at 43°C for 1 h. ^111^In-DOTA-T84.66 minibody was isolated with gel filtration through a column with a radiochemical purity of >98%. The overall radiochemical yields were 24–85%. The specific activity was 7–13 GBq/μmol (184–376 mCi/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20in%20vitro)]

Radioimmunoreactivity of ^111^In-DOTA-T84.66 minibody for recombinant CEA was determined with size-exclusion high-performance liquid chromatography analysis to be 70–100% (14). The affinity constant of DOTA-T84.66 minibody was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20rodentia)]

Yazaki et al. (14) performed biodistribution studies of ^111^In-DOTA-T84.66 minibody in nude mice (n = 5 mice/group) with the use of an LS174T subcutaneous xenograft model. Data were obtained at 2, 6, 12, 24, 48, and 72 h after injection. ^111^In-DOTA-T84.66 minibody had a rapid blood clearance, resulting in low activity in the blood at 2, 12, and 24 h (17.74 ± 0.79%, 3.61 ± 0.59%, and 0.60 ± 0.04% injected dose (ID)/g, respectively). The blood clearance pattern exhibited a two-phase model with a half-life of 0.42 h during the distribution phase and a half-life of 4.51 h during the elimination phase. The tracer accumulation in the CEA-expressing tumor was 14.2 ± 6.1% ID/g at 2 h, 24.47 ± 6.1% ID/g at 12 h, 18.84 ± 1.17% ID/g at 24 h, and 11.33 ± 0.95% ID/g at 48 h. The liver had the highest accumulation with a peak of 25.97 ± 0.99% ID/g at 24 h. All other major organs exhibited lower levels of radioactivity than the tumor. Renal accumulation reached a plateau of 12–13% ID/g, which decreased to 7.2% ID/g at 72 h. The tumor/blood ratio increased significantly over time (0.8, 7, 32, and 109 at 2, 12, 24, and 48 h after injection, respectively). The tumor/liver ratio of 1.36 peaked at 12 h. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20human)]

No publication is currently available.

## NIH Support

P01 CA43904, CA33572

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.
15 Yazaki P.J., Shively L., Clark C., Cheung C.W., Le W., Szpikowska B., Shively J.E., Raubitschek A.A., Wu A.M. (2001). Mammalian expression and hollow fiber bioreactor production of recombinant anti-CEA diabody and minibody for clinical applications. J Immunol Methods.